# ^111^In-Trastuzumab Fab

Chemical name: | ^111^In-Trastuzumab Fab
Abbreviated name: | ^111^In-humAb4D5-8 Fab
Synonym: | ^111^In-Herceptin^®^ Fab, ^111^In-anti-HER2 MAb Fab
Agent Category: | Antibody
Target: | Human epidermal growth factor receptor 2 (HER2)
Target Category: | Antibody to antigen binding
Method of detection: | SPECT, planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=119533), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=183984) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064) for more information about VEGF

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-trastuzumab%20OR%20111In-Herceptin%29)]

^111^In-Trastuzumab Fab (^111^In-humAb4D5-8 Fab) is formed by the conjugation of ^111^In via the bifunctional chelate, diethylenetriamine pentaacetic acid (DTPA), with the Fab fragment of the recombinant humanized monoclonal antibody (MAb) against the antigen of human epidermal growth factor receptor 2 (HER2). ^111^In-Trastuzumab Fab has been developed for imaging of human breast cancer (1-3).

The epidermal growth factor receptors (HER/erbB) with tyrosine kinase activity are involved in transmission of signals controlling normal cell development, growth, differentiation, and survival (2, 4, 5). This cell surface receptor family consists of four distinct members: the epidermal growth factor receptors HER1, HER2, HER3, and HER4. These receptors are found in various combinations in different tissues. There are nine ligands that bind directly to HER1, HER3, or HER4, and HER2 can be activated as a result of ligand binding to other HER receptors. The ligandless HER2 receptor is encoded by the human gene HER2/c-erbB2 (HER2/neu). It has been found to be overexpressed in a wide variety of human cancers and in 20-30% of primary breast cancers (6). This overexpression is associated with aggressive tumor growth and metastatic activity. In breast cancer, HER2/neu gene amplification can result in 10- to 100-fold higher HER2 protein levels in tumor cells than in normal breast epithelium. HER2 overexpression is considered a negative prognostic indicator for breast cancer.

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (7-9). Anti-HER2 MAbs have been generated for inhibiting the growth of tumor cells possessing activated HER2/neu receptors (10). Murine 4D5 MAb was raised against human breast and ovarian tumor cell lines overexpressing p185^HER2^. This MAb was found to recognize an extracellular epitope (amino acids 529 to 627) in the cysteine-rich II domain that resides very close to the transmembrane region (10). Murine 4D5 MAb was fully humanized by Carter et al. (11) to generate humAb4D5-8 MAb in an effort to improve the safety and tolerance of the antibody for clinical applications. Trastuzumab is of the immunoglobulin G_1_ (IgG_1_) kappa class and binds to the recombinant HER2 extracellular domain with an affinity (K_d_) of 0.1 nM. However, the pharmacokinetics of intact radiolabeled IgG, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Clinically, cardiotoxicity is the most serious complication of using trastuzumab in humans (6, 12). One potential application of a radiolabeled anti-HER2 MAb is the pretreatment imaging of breast cancer patients to predict the cardiotoxicity and therapeutic efficacy of unlabeled trastuzumab.

Various anti-HER2 MAbs have been labeled with ^131^I, ^125^I, ^111^In, ^86^Y, ^90^Y, ^64^Cu, ^76^Br, or Gd for potential imaging and therapy applications (1, 13-19). Labeling with radiometals is generally achieved by indirect labeling with use of a bifunctional chelating agent (20, 21). ^111^In, a photon emitter with a physical half-life of 2.8 days, is considered one of the radionuclides of choice for antibody imaging studies.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28111In%5BAll%20Fields%5D%20AND%20%28%22trastuzumab%22%5BSubstance%20Name%5D%20OR%20Trastuzumab%5BText%20Word%5D%29%29%20OR%20111In-Herceptin%5BAll%20Fields%5D%29%20AND)]

Trastuzumab was synthesized by humanization of murine 4D5 MAb (11). The complementarity determining regions of murine 4D5 MAb were transplanted into a human antibody model. A final “humanized” antibody, humAb4D5, containing only the antigen-binding loops from murine 4D5 MAb and human variable region framework residues plus IgG_1_ constant domains, was constructed. HumAb4D5-8 was found to bind its antigen 3-fold more tightly than the murine 4D5 MAb. Lub-de Hooge et al (2) described radiolabeling of the intact humAb4D5-8 MAb with ^111^In by conjugation using a modified cyclic DTPA anhydride method (2, 21).

Tang et al. (3) prepared the trastuzumab Fab fragments by digestion of trastuzumab. The intact MAb was reacted with a 1/10 amount (by weight) of immobilized papain for 20 min at 37 °C under nitrogen in a 20 mM sodium phosphate buffer with cysteine and edetate disodium. After digestion, the Fab fragment was collected by ultrafiltration in a final concentration of 5.0 mg/ml. The yield was 45%. The purity was determined by sodium dodecyl sulfate--polyacrylamide gel electrophoresis, Western blotting, and size-exclusion high-performance liquid chromatography. Trastuzumab Fab migrated with a molecular mass of 47 kDa, and the purity was >90%. For radiolabeling, trastuzumab Fab was derivatized with the bifunctional chelator DTPA by incubating in10-fold molar excess of DTPA dianhydride in 50 mM sodium bicarbonate buffer (pH 8.0) for 30 min at room temperature (3). Excess DTPA was removed by Sephadex G-25 filtration, and 2.6 ± 0.3 molecules of DTPA were introduced into each molecule of trastuzumab Fab. Purified DTPA-trastuzumab Fab was radiolabeled by incubation with 18.5 MBq (0.5 mCi)/5 µl of ^111^In acetate for 30 min at room temperature. ^111^In-Trastuzumab Fab was purified by Sephadex G-25 column. The radiochemical purity was >98%, and the specific activity was 48-74 kBq (1.29-2 µCi)/µg (2.26-3.49 kBq (0.06-0.09 µCi)/µmol based on a molecular mass of 47 kDa).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20in%20vitro)]

Tang et al. (3) evaluated the immunoreactivity of the Fab and compared it with that of intact trastuzumab. This was done by saturation and competition receptor-binding assays using HER2/neu-positive SK-BR-3 human breast cancer cells. The affinity (K_d_) of the Fab from the saturable receptor binding assay was 1.4 ± 0.2 × 10−^8^ M compared with 7.7 ± 2.0 × 10−^9^ M for intact trastuzumab. The maximum number of receptors per cell (B_max_) was 2.9 ± 0.12 × 10^6^ for the trastuzumab Fab compared with 2.0 ± 0.23 × 10^6^ for intact trastuzumab. In the competition receptor-binding assays, trastuzumab Fab competed specifically with ^125^I-trastuzumab IgG for binding to SK-BR-3 cells. The K_d_ for trastuzumab Fab was 3.6 ± 1.4 × 10−^8^ M compared with 1.4 ± 0.2 × 10−^8^ M for intact trastuzumab and 4.7 ± 2.3 × 10−^8^ M. for the DTPA-trastuzumab Fab.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20rodentia)]

Tang et al. (3) performed biodistribution studies of ^111^In-trastuzumab Fab in athymic nude mice bearing s.c. HER2/neu-positive BT-474 human breast cancer xenografts (1-2 × 10^6^ receptors/cell). Each tumor-bearing mouse received 1.1 MBq (0.03 mCi)/30 µg of ^111^In-trastuzumab Fab. Posterior whole-body images were obtained with a dose of 3.7 MBq (0.5 mCi)/30 µg. The blood activity rapidly decreased from 1.4 ± 0.39 (n = 4-5) percent of injected dose (% ID)/g at 24 h to 0.3 ± 0.01% ID/g at 72 h. The tumor radioactivity increased from 5.2 ± 1.49% ID/g at 24 h to 7.8 ± 0.70% ID/g at 72 h. Small tumors (3-5 mm in diameter) were visualized as early as 24 h after injection. The tumor/blood ratio increased from 4.2 ± 0.64 at 24 h to 25.2 ± 1.62 at 72 h. Other tumor/nontumor ratios increased over a 72-h period with the highest ratios for tumor/muscle (13. 6 ± 2.16) and tumor/stomach (19.4 ± 4.51). The kidney was the critical organ, with 53.0 ± 15.94% ID/g at 24 h and 83.8 ± 6.98% ID/g at 72 h. In comparison, the liver had only 2.4 ± 0.79% ID/g at 24 h and 2.9 ± 0.29% ID/g at 72 h. The radioactivity concentrations at 24 h for the heart, lung, and spleen were 1.1 ± 0.32, 1.8 ± 0.55, and 3.5 ± 1.18% ID/g, respectively. At 72 h, these values were 1.2 ± 0.42, 1.6 ± 0.19, and 4.7 ± 0.56% ID/g, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28111In-Trastuzumab%20OR%20111In-Herceptin%29%20AND%20human)]

No publication is currently available.

## References

1 Garmestani K, Plascjak PS, Brechbiel MW. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
2 Lub-de Hooge MN, Kosterink JG, Perik PJ, Nijnuis H, Tran L, Bart J, Suurmeijer AJ, de Jong S, Jager PL, de Vries EG. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
3 Tang Y, Wang J, Scollard DA, Mondal H, Holloway C, Kahn HJ, Reilly RM. (2005). Imaging of HER2/neu-positive BT-474 human breast cancer xenografts in athymic mice using (111)In-trastuzumab (Herceptin) Fab fragments. Nucl Med Biol.
4 Frankel C Development and clinical overview of trastuzumab (herceptin) Semin Oncol Nurs 2000 16 4 Suppl 1 13 17 11151453
5 Sliwkowski MX Lofgren JA Lewis GD Hotaling TE Fendly BM Fox JA Nonclinical studies addressing the mechanism of action of trastuzumab (Herceptin) Semin Oncol 1999 26 4 Suppl 12 60 70 10482195
6 Slamon DJ, Leyland-Jones B, Shak S, Fuchs H, Paton V, Bajamonde A, Fleming T, Eiermann W, Wolter J, Pegram M, Baselga J, Norton L. (2001). Use of chemotherapy plus a monoclonal antibody against HER2 for metastatic breast cancer that overexpresses HER2. N Engl J Med.
7 Wu AM, Senter PD. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
8 Brechbiel MW. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
9 Kowalsky RJ, Falen SW. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , : APhA. 733-752.
10 Fendly BM, Winget M, Hudziak RM, Lipari MT, Napier MA, Ullrich A. (1990). Characterization of murine monoclonal antibodies reactive to either the human epidermal growth factor receptor or HER2/neu gene product. Cancer Res.
11 Carter P, Presta L, Gorman CM, Ridgway JB, Henner D, Wong WL, Rowland AM, Kotts C, Carver ME, Shepard HM. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Behr TM, Behe M, Wormann B. (2001). Trastuzumab and breast cancer. N Engl J Med.
13 Blend MJ, Stastny JJ, Swanson SM, Brechbiel MW. (2003). Labeling anti-HER2/neu monoclonal antibodies with 111In and 90Y using a bifunctional DTPA chelating agent. Cancer Biother Radiopharm.
14 Olafsen T, Kenanova VE, Sundaresan G, Anderson AL, Crow D, Yazaki PJ, Li L, Press MF, Gambhir SS, Williams LE, Wong JY, Raubitschek AA, Shively JE, Wu AM. (2005). Optimizing radiolabeled engineered anti-p185HER2 antibody fragments for in vivo imaging. Cancer Res.
15 Winberg KJ, Persson M, Malmstrom PU, Sjoberg S, Tolmachev V. (2004). Radiobromination of anti-HER2/neu/ErbB-2 monoclonal antibody using the p-isothiocyanatobenzene derivative of the [76Br]undecahydro-bromo-7,8-dicarba-nido-undecaborate(1-) ion. Nucl Med Biol.
16 Xu FJ, Yu YH, Bae DS, Zhao XG, Slade SK, Boyer CM, Bast RC, Zalutsky MR. (1997). Radioiodinated antibody targeting of the HER-2/neu oncoprotein. Nucl Med Biol.
17 Palm S, Enmon RM, Matei C, Kolbert KS, Xu S, Zanzonico PB, Finn RL, Koutcher JA, Larson SM, Sgouros G. (2003). Pharmacokinetics and Biodistribution of (86)Y-Trastuzumab for (90)Y dosimetry in an ovarian carcinoma model: correlative MicroPET and MRI. J Nucl Med.
18 Tsai SW, Sun Y, Williams LE, Raubitschek AA, Wu AMJE. (2000). Biodistribution and radioimmunotherapy of human breast cancer xenografts with radiometal-labeled DOTA conjugated anti-HER2/neu antibody 4D5. Bioconjug Chem.
19 Kobayashi H, Shirakawa K, Kawamoto S, Saga T, Sato N, Hiraga A, Watanabe I, Heike Y, Togashi K, Konishi J, Brechbiel MW, Wakasugi H. (2002). Rapid accumulation and internalization of radiolabeled herceptin in an inflammatory breast cancer xenograft with vasculogenic mimicry predicted by the contrast-enhanced dynamic MRI with the macromolecular contrast agent G6-(1B4M-Gd)(256). Cancer Res.
20 Fritzberg AR, Berninger RW, Hadley SW, Wester DW. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
21 Hnatowich DJ, Childs RL, Lanteigne D, Najafi A. (1983). The preparation of DTPA-coupled antibodies radiolabeled with metallic radionuclides: an improved method. J Immunol Methods.